# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-β max tris(acetic acid)-10-acetate mono(N-ethylmaleimide amide)-dimeric (Z_HER2:477_)_2_

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-β max tris(acetic acid)-10-acetate mono(N-ethylmaleimide amide)-dimeric (Z_HER2:477_)_2_ | [image]
Abbreviated name: | ^64^Cu-DOTA-(Z_HER2:477_)_2_ | [image]
Synonym: | | [image]
Agent Category: | Affibody, antibody | [image]
Target: | HER2 | [image]
Target Category: | Receptor | [image]
Method of detection: | PET | [image]
Source of signal / contrast: | ^64^Cu | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of the agents by Cheng et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

The ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7-β max tris(acetic acid)-10-acetate mono(N-ethylmaleimide amide) (Mal-DOTA)-dimeric (Z_HER2:477_)_2_ conjugate, abbreviated as ^64^Cu-DOTA-(Z_HER2:477_)_2_, is an affibody derivative synthesized by Cheng et al. for positron emission tomography (PET) of HER2-expressing tumors (1).

Affibody molecules are a group of nonimmunogenic scaffold proteins that derive from the B-domain of staphylococcal surface protein A (2, 3). In the past several years, affibodies have drawn significant attention for developing imaging and therapeutic agents because of their unique features (3, 4). First, affibodies are small, with only 58 amino acid residues (~7 kDa) (3, 5). The small size allows affibodies to be generated with solid-phase peptide synthesis and to be cleared quickly from kidneys. Second, affibodies have a high binding affinity and specificity to their targets. Their binding affinity can be further improved by generating multimeric constructs through the solvent-exposed termini of affibody Z-domain. The anti-HER2 monomeric affibody Z_HER2:4_ is an example that has a binding affinity of ~50 nM, but its dimeric form, (Z_HER2:4_)_2_, exhibits an improved binding affinity up to ~3 nM (6). Third, affibodies lack cysteine residues and disulfide bridges in structure, and they fold rapidly. These features make it possible to chemically synthesize fully functional molecules and to introduce unique cysteine residues or chemical groups into affibodies for site-specific labeling. Several anti-HER2 affibody derivatives have been synthesized in this way. The imaging agent HPEM-His_6_-(Z_HER2:4_)_2_-Cys was generated by radiobrominating the dimeric (Z_HER2:4_)_2_ through the cysteine residues that were introduced to the C-terminus of (Z_HER2:4_)_2_ (7). Several affibody derivatives (e.g., ^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), and ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/)) were synthesized by coupling a chelating agent with a specifically protected site group of the Z_HER2:342_ peptide chain (3). Furthermore, these small affibody proteins can be selected and optimized with a strategy of sequence mutation and affinity maturation, and an example selected with this strategy is the anti-HER2 affibody Z_HER2:342_, which has an increased affinity from 50 nM to 22 pM (8).

The investigators at the Stanford University first tested the feasibility of the monomeric and dimeric forms of affibody Z_HER2:477_ for molecular imaging. Z_HER2:477_ is a commercially available anti-HER2 affibody. Both forms of the Z_HER2:477_ molecule were radiofluorinated with an ^18^F-labeled prosthetic group of 4-^18^F-fluorobenzaldehyde (^18^F-FBO-Z_HER2:477_ and ^18^F-FBO-(Z_HER2:477_)_2_, respectively) (9). The investigators have also coupled ^64^Cu to the affibody through DOTA, leading to the development of imaging agents of ^64^Cu-DOTA- Z_HER2:477_ and ^64^Cu-DOTA-(Z_HER2:477_)_2_ (1). Interestingly, these studies showed that smaller affibody constructs performed better in vivo in terms of tumor uptake and clearance. The investigators then generated a class of small proteins consisting of two α-helix bundles of the 3-helix affibody by deleting the helix 3 because the binding domain localizes in the α-helices 1 and 2 bundles (5). One of these 2-helix proteins is MUT-DS, which has α-helices 1 and 2 bundles, with a disulfide bridge being formed between the two inserted homocysteines (10-12). The helix conformation of MUT-DS has been shown to be improved with the placement of a disulfide bridge. MUT-DS showed a binding affinity to HER2 in the low-nM range. The radiolabeled MUT-DS derivatives exhibited favorable pharmacokinetics for both imaging and therapy of HER2-expressing tumors.

This series of chapters summarizes the data obtained with the Z_HER2:477_ derivatives, and this chapter presents the data obtained with ^64^Cu-DOTA-(Z_HER2:477_)_2_ (1).

### Related Resource Links:

- Anti-HER2 affibody conjugates in MICAD:

^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), Alexa750-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK45127/), ^111^In-Benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), ^111^In-Benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/), Eaff800 (http://www.ncbi.nlm.nih.gov/books/NBK45665/), DY-682-ABD-Z_HER2:342_ (Haff682) (http://www.ncbi.nlm.nih.gov/books/NBK45664/), ^99m^Tc-Z_2395_-C (http://www.ncbi.nlm.nih.gov/books/NBK23590/), [^111^In]-ABY-025 (http://www.ncbi.nlm.nih.gov/books/NBK45623/), ^111^In-BZ-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/).

- HER2-related clinical trials for imaging and therapy (http://clinicaltrials.gov/ct2/results?term=HER2)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The dimeric affibody (Z_HER2:477_)_2_ with a purity of >95% is commercially available. The maleimide-functionalized chelator, Mal-DOTA, was synthesized with DOTA-mono-NHS-tris(tBu)ester, triethylamine, and N-(2-aminoethyl)maleimide-trifluoroacetic acid salt. The affibody (Z_HER2:477_)_2_ was then modified at the cysteine residue of the C terminus with Mal-DOTA, which generated the conjugate DOTA-(Z_HER2:477_)_2_ (1). The molecular weight of DOTA-(Z_HER2:477_)_2_ was 14,563.81 Da with 47% recovery yield after purification. The conjugate was radiolabeled with ^64^Cu by incubation with ^64^CuCl_2_ for 1 h at 40°C. The product, ^64^Cu-DOTA-(Z_HER2:477_)_2_, was purified on a PD-10 column and analyzed with radioanalytical high-performance liquid chromatography (HPLC).

The final product, ^64^Cu-DOTA-(Z_HER2:477_)_2_, had a radiochemical purity of >95% and a specific activity of 115.3 MBq/nmol (3.12 mCi/nmol). HPLC analysis of the ^64^Cu-DOTA-(Z_HER2:477_)_2_ showed a single peak with a retention time of 21.6 min. Octanol–water partition coefficient measurements showed a logP value of −0.46 ± 0.04, indicating intermediate hydrophilicity of the ^64^Cu-DOTA-(Z_HER2:477_)_2_ (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

Binding affinity with the extracellular domain of HER2 antigen was measured in vitro with surface plasmon resonance detection (1). Unlabeled DOTA-(Z_HER2:477_)_2_ showed a binding affinity of 100 pM (for 1.5 nM DOTA-Z_HER2:477_) with association constants in the range of 10^5^ and dissociation constants in the range of 10−^4^–10−^5^, indicating that the on rate was very fast and the off rate was very slow. Binding affinity for ^64^Cu-DOTA-(Z_HER2:477_)_2_ was not measured.

HER2 expression in SKOV3 human ovarian and MDA-MB-435 human breast cancer cells and tumor samples was verified with Western blot analysis (1). SKOV3 cells had high HER2 expression, whereas MDA-MB-435 cells expressed minimum HER2. The HER2 expression was 10–15-fold higher in SKOV3 tumors than in MDA-MB-435 tumors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Biodistribution studies were performed in nude mice bearing SKOV3 tumors (n = 3 mice/time point) (1). Mice were injected via the tail vein with 0.185–0.37 MBq (5–10 µCi) ^64^Cu-DOTA-(Z_HER2:477_)_2_ and euthanized at 1, 4, and 20 h after injection, respectively. The radioactivity in ex vivo tissues was expressed as a percentage of the injected radioactive dose per gram of tissue (% ID/g). ^64^Cu-DOTA-(Z_HER2:477_)_2_ exhibited rapid accumulation with moderate activity in the SKOV3 tumors at the early time point (2.01 ± 0.46% ID/g at 1 h), which then decreased to 1.46 ± 0.50% ID/g and 1.53 ± 0.35% ID/g at 4 h and 20 h after injection, respectively. The tumor/blood ratios were 0.91 ± 0.33, 2.00 ± 0.69, and 2.06 ± 0.04, and the tumor/muscle ratios were 3.44 ± 0.66, 3.96 ± 1.43, and 4.43 ± 1.02 at 1, 4, and 20 h, respectively.

Comparison between ^64^Cu-DOTA-Z_HER2:477_ and its dimeric form ^64^Cu-DOTA-(Z_HER2:477_)_2_ showed that ^64^Cu-DOTA-Z_HER2:477_ had much higher tumor uptake than ^64^Cu-DOTA-(Z_HER2:477_)_2_ at all time points (P < 0.05). Both forms displayed rapid blood clearance, with 0.75 ± 0.22% ID/g and 2.27 ± 0.27% ID/g blood uptake at 1 h for ^64^Cu-DOTA-Z_HER2:477_ and ^64^Cu-DOTA-(Z_HER2:477_)_2_, respectively. Extremely high renal uptake and retention were found for both forms, but the renal uptake for monomeric ^64^Cu-DOTA-Z_HER2:477_ was 1–1.5-fold higher than that for ^64^Cu-DOTA-(Z_HER2:477_)_2_. The renal uptake values at 1, 4, and 20 h were 206.26 ± 22.36%, 237.51 ± 34.49%, and 129.69 ± 14.43% ID/g for ^64^Cu-DOTA-Z_HER2:477_ and 114.33 ± 11.22%, 75.21 ± 5.74%, and 37.95 ± 5.55% ID/g for ^64^Cu-DOTA-(Z_HER2:477_)_2_, respectively. Although relatively high liver uptake was observed for both agents, it was much lower than the renal uptake. Both forms exhibited relatively low uptake in all other normal organs.

PET imaging was performed in a mouse bearing SKOV3 and MDA-MB-435 tumors at 1, 4, and 20 h after tail vein injection of ^64^Cu-DOTA-(Z_HER2:477_)_2_ (1). SKOV3 tumor was visible with moderate tumor/background contrast at 1–20 h after injection. Very poor uptake was observed in the MDA-MB-435 tumor, which makes it difficult to be visualized. Consistent with the biodistribution findings, high radioactivity accumulation was observed in the kidneys.

In conclusion, the ^64^Cu-labeled dimer and monomer exhibited rapid tumor accumulation and blood clearance, which are favorable for imaging (1). Although the dimeric form exhibited higher HER2-binding affinity than did the monomeric form, the dimeric form showed much lower SKOV3 tumor accumulation and tumor/normal organ ratios than that of the monomeric form. Very high kidney uptake and retention for both agents are likely to be a concern for their clinical use, and further optimization is necessary (1). Blocking studies were not performed for the dimeric form, although Herceptin blocked the binding of ^64^Cu-DOTA-Z_HER2:477_.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Cheng Z., De Jesus O.P., Kramer D.J., De A., Webster J.M., Gheysens O., Levi J., Namavari M., Wang S., Park J.M., Zhang R., Liu H., Lee B., Syud F.A., Gambhir S.S. (2010). 64Cu-labeled affibody molecules for imaging of HER2 expressing tumors. Mol Imaging Biol.
2 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
3 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
4 Tolmachev V., Orlova A., Nilsson F.Y., Feldwisch J., Wennborg A., Abrahmsen L. (2007). Affibody molecules: potential for in vivo imaging of molecular targets for cancer therapy. Expert Opin Biol Ther.
5 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
6 Steffen A.C., Wikman M., Tolmachev V., Adams G.P., Nilsson F.Y., Stahl S., Carlsson J. (2005). In vitro characterization of a bivalent anti-HER-2 affibody with potential for radionuclide-based diagnostics. Cancer Biother Radiopharm.
7 Mume E., Orlova A., Larsson B., Nilsson A.S., Nilsson F.Y., Sjoberg S., Tolmachev V. (2005). Evaluation of ((4-hydroxyphenyl)ethyl)maleimide for site-specific radiobromination of anti-HER2 affibody. Bioconjug Chem.
8 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
9 Cheng Z., De Jesus O.P., Namavari M., De A., Levi J., Webster J.M., Zhang R., Lee B., Syud F.A., Gambhir S.S. (2008). Small-animal PET imaging of human epidermal growth factor receptor type 2 expression with site-specific 18F-labeled protein scaffold molecules. J Nucl Med.
10 Ren, G., J.M. Webster, Z. Liu, R. Zhang, Z. Miao, H. Liu, S.S. Gambhir, F.A. Syud, and Z. Cheng, In vivo targeting of HER2-positive tumor using 2-helix affibody molecules. Amino Acids, 2011
11 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.
12 Miao Z., Ren G., Jiang L., Liu H., Webster J.M., Zhang R., Namavari M., Gambhir S.S., Syud F., Cheng Z. (2011). A novel (18)F-labeled two-helix scaffold protein for PET imaging of HER2-positive tumor. Eur J Nucl Med Mol Imaging.